# Recombinant human erythropoietin coupled to near-infrared fluorescence dye Cy5.5

Chemical name: | Recombinant human erythropoietin coupled to near-infrared fluorescence dye Cy5.5
Abbreviated name: | Epo-Cy5.5
Synonym:
Agent Category: | Protein (glycoprotein)
Target: | Erythropoietin receptor (Epo-R)
Target Category: | Receptor
Method of detection: | Optical imaging (fluorescence-mediated tomography (FMT))
Source of signal / contrast: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=erythropoietin%20and%20cancer&cmd=DetailsSearch)]

Erythropoietin (Epo) is a heavily glycosylated chemokine that is expressed primarily in the adult kidney (during the fetal stage of development, Epo is produced mainly in the liver and not the kidneys), mediates its effects through the erythropoietin receptor (Epo-R), and is known to regulate the process of erythropoiesis (red blood cell formation from hematopoietic cells in the bone marrow) in the hematopoietic system (1). Epo-R is also found in other tissues and is believed to protect cells in the cardiac and neuronal tissues from hypoxic injury and apoptosis. The expression of Epo and Epo-R and the cell signaling pathways involved in bringing about the biological effects of this receptor-ligand complex have been described by Chateauvieux et al. (1). The use of recombinant human Epo (rhuEpo) has been approved by the United States Food and Drug Administration for the treatment of anemia (http://dailymed.nlm.nih.gov/dailymed/lookup.cfm?setid=1f2d0b28-9cc5-4523-80b8-637fdaf3f7a5#nlm34067-9) in certain HIV patients and individuals undergoing chemotherapy for non-myeloid cancer or those who are experiencing chronic kidney failure. Meta-analysis of data obtained from clinical trials has shown that the use of rhuEpo in the clinic is associated with increased adverse thrombo-vascular events or neoplastic tumor progression that results in the mortality of individuals with certain types of cancer (2). In a mouse model of breast cancer it has been shown that, when rhuEpo was used in combination with chemotherapy, there was an increased incidence of cancer metastasis in the animals (3). The co-expression of Epo and Epo-R has been observed in certain neoplasms, including non-small cell lung cancer (NSCLC), and a clinical investigation has shown that expression of these genes in the NSCLC tumors correlated with a negative outcome for the patient (4). However, other studies could not establish a clear link between the expression of Epo and Epo-R and the development of cancer because the Epo-R status of a tumor cannot be determined accurately with currently used immunohistochemical methods, due to the lack of antibodies that can specifically and selectively bind to the Epo-R (5). Therefore, the development of alternative probes that specifically target the Epo-R and can be used with noninvasive imaging techniques to detect and quantify the receptor in vivo is necessary (5). Doleschel et al. coupled Cy5.5, a near-infrared dye, to rhuEpo (Epo-Cy5.5) and evaluated the fluorescent conjugate to visualize the expression of EpoR with fluorescence-mediated tomography (FMT) in human lung cancer xenografts in mice (5). The biodistribution of the probe in these animals was also investigated.

### Related Resource Links

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Erythropoietin) related to erythropoietin

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_021395.1) and protein (http://www.ncbi.nlm.nih.gov/protein/AAA52403.1) sequences of human erythropoietin receptor

Erythropoietin receptor in Online Mendelian Inheritance in Man (OMIM) Database (http://omim.org/entry/133171)

Human hematopoietic cell lineage pathways (http://www.genome.jp/dbget-bin/www_bget?hsa04640) (from Kyoto Encyclopedia of Genes and Genomes)

Anemia (http://kidney.niddk.nih.gov/kudiseases/pubs/anemia/) in kidney disease and dialysis

Information about non-small cell lung cancer (http://www.cancer.gov/cancertopics/pdq/treatment/non-small-cell-lung/healthprofessional) (from National Cancer Institute website)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epo%20Cy5.5%20synthesis&cmd=DetailsSearch)]

A commercially available kit of Cy5.5 was used to couple the dye to the free carbonyl groups of the periodate-oxidized carbohydrate side chains of rhuEpo (5). Information regarding the source of rhuEpo used to produce Epo-Cy5.5, the purification, purity, and yield of the final fluorescent product, and the number of Cy5.5 molecules attached to each molecule of rhuEpo was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epo%20Cy5.5%20in%20vitro&cmd=DetailsSearch)]

Epo-Cy5.5 and rhuEpo were reported to generate a similar dose-dependent proliferation curve with UT-7 cells (the proliferation of this human acute myeloid leukemia cell line is Epo dependent), indicating that the biological activity of the Cy5.5 conjugate was the same as the parent molecule (5).

NSCLC cell lines A549 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-185&Template=cellBiology), H838 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-5844&Template=cellBiology), and H2030 (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CRL-5914&Template=cellBiology) were used to determine the in vitro binding specificity of Epo-Cy5.5 (5). Before performing the binding study, the expression of Epo-R mRNA and protein in these cell lines was confirmed with quantitative RT-PCR and quantitative immunoblotting, respectively (5). The expression of Epo-R was reported to be higher in the H838 cells (~2000 Epo-R protein/cell) compared with the A549 cells (~250 Epo-R protein/cell), and the H2030 cells did not express any Epo-R. The NSCLC cell lines were exposed to Epo-Cy5.5, and fluorescence microscopy of the different cells at the same exposure times revealed that the fluorescence signal generated by the H838 cells was higher than that generated by the A549 cells, and no signal was observed with the H2030 cells. This indicated that Epo-Cy5.5 had a high binding specificity for Epo-R on these cells.

To further confirm the Epo-R binding specificity of Epo-Cy5.5, Epo-R/enhanced green fluorescence protein (EGFP)-transfected HeLa (https://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-2&Template=cellBiology) cells (Epo-R/EGFP is a fusion protein that has EGFP fused to the C-terminal of the Epo-R; these cells overexpress the fusion protein) were exposed to Epo-Cy5.5 (10 nM) in the absence or presence of excess (190 nM) unlabeled rhuEpo (5). Fluorescence microscopy of the two groups of cells showed that cells incubated with Epo-Cy5.5 alone had a significantly higher (P < 0.05) signal intensity compared with cells incubated with Epo-Cy5.5 in the presence of unlabeled rhuEpo. These observations again indicated that Epo-Cy5.5 had a high specificity of binding to the Epo-R (5).

In another study, cryosections of A549 and H838 cell xenograft tumors in nude mice (see below for details) were exposed to Epo-Cy5.5 and examined under a fluorescent microscope (5). Muscle sections obtained from the same animals were used as controls because this tissue does not express Epo-R. A fluorescence signal was detected only in the tumor sections, and the H838 tumor cells generated a stronger signal compared to cells from the A549 lesions. From these observations, the investigators concluded that the level of fluorescence signal generated by the tumor cells correlated with the degree of Epo-R expression in these cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epo%20Cy5.5%20rodentia&cmd=DetailsSearch)]

To determine the in vivo specificity of Epo-Cy5.5, nude mice bearing xenograft tumors generated with either A549 or H838 cells were injected with the conjugate (n = 4 animals/group per cell line) through the tail vein as described by Doleschel et al. (5). Control animals were injected with Epo-Cy5.5 alone (10 μM), and the competition group received a 1:5 mixture of Epo-Cy5.5/rhuEpo (10 μM:40 μM). Micro-computed tomographic (micro-CT)/FMT images were acquired simultaneously from the anesthetized mice at 0.5, 3, 5, 7, 23, 30, 48, and 50 h postinjection (p.i.), and the concentration of Epo-Cy5.5 in tissues of interest was determined by using appropriate software. In general, the tumors of both cell lines in animals injected with Epo-Cy5.5 alone showed a higher concentration of the conjugate at all the time points compared with tumors in mice of the competition group. At 5 h and 7 h p.i., the A549 tumors of control animals had a significantly higher concentration of Epo-Cy5.5 compared with tumors of the competition group (57.4 ± 18.3 nM versus 21.68 ± 8.67 nM; P < 0.05), and a similar difference was apparent at 25 h p.i. The H838 tumors in the control animals showed a significantly higher concentration (P < 0.001) of the fluorescent conjugate from 7 h to 48 h p.i. compared with the competition group (93.96 ± 11.39 nM and 32.44 ± 7.64 nM, respectively). These observations indicated that the Epo-Cy5.5 probe bound specifically to the Epo-R in these tumors. Micro-CT/FMT fusion images of the H838 control mice acquired at 50 h p.i. showed a higher accumulation of the probe compared with the competition animals, but the bone marrow from animals of both groups had a similar concentration of Epo-Cy5.5. The investigators observed that the amount of Cy5.5-conjugated Epo in the H838 and the A549 cell tumors correlated with the level of Epo-R expression in these cells.

The biodistribution of Epo-Cy5.5 was investigated in mice bearing A549 cell tumors (5). The animals were injected with the probe as described above, and micro-CT/FMT images were acquired from the animals up to 50 h p.i. The tracer was present in the blood at high levels immediately after injection, and the levels decreased gradually during the next 3 h p.i., followed by a relatively constant level for up to 50 h p.i. Between 3 h and 7 h p.i., the maximum accumulation of the fluorescent conjugate was observed in the liver followed by the kidneys (416.77 ± 135.28 nM and 377.75 ± 227.14 nM, respectively); subsequently, the kidneys showed a gradual decrease in the levels of Epo-Cy5.5 (~100 nM at 50 h p.i.), whereas in the liver the concentration decreased gradually up to 24 h p.i. and stayed relatively constant (~ 200 nM) up to 50 h p.i. The amount of Epo-Cy5.5 in the bone marrow stayed almost constant from 3 h to 50 h p.i. (average concentration 98.24 ± 8.77 nM).

From these studies it was concluded that Epo-Cy5.5 can be used to investigate the expression of Epo-R in tumors and the role of this cytokine in the progression of experimental cancerous tumors in mice (5).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epo%20Cy5.5%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epo%20Cy5.5%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=Epo%20Cy5.5%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Chateauvieux S., Grigorakaki C., Morceau F., Dicato M., Diederich M. (2011). Erythropoietin, erythropoiesis and beyond. Biochem Pharmacol.
2 McKinney M., Arcasoy M.O. (2011). Erythropoietin for oncology supportive care. Exp Cell Res.
3 Hedley B.D., Chu J.E., Ormond D.G., Beausoleil M.S., Boasie A., Allan A.L., Xenocostas A. (2011). Recombinant human erythropoietin in combination with chemotherapy increases breast cancer metastasis in preclinical mouse models. Clin Cancer Res.
4 Rades D., Setter C., Dahl O., Schild S.E., Noack F. (2011). Prognostic impact of erythropoietin expression and erythropoietin receptor expression on locoregional control and survival of patients irradiated for stage II/III non-small-cell lung cancer. Int J Radiat Oncol Biol Phys.
5 Doleschel D., Mundigl O., Wessner A., Gremse F., Bachmann J., Rodriguez A., Klingmuller U., Jarsch M., Kiessling F., Lederle W. (2012). Targeted Near-Infrared Imaging of the Erythropoietin Receptor in Human Lung Cancer Xenografts. J Nucl Med.